# Microbubbles coated with biotinylated rabbit anti-mouse endoglin monoclonal antibody

Chemical name: | Microbubbles coated with rabbit anti-mouse endoglin monoclonal antibody
Abbreviated name: | MB_endoglin_
Synonym:
Agent Category: | Antibody
Target: | Endoglin
Target Category: | Antigen
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Ultrasound%20microbubbles&cmd=DetailsSearch)]

Angiogenesis, the development of new vasculature from pre-existing blood vessels (for details see Carmeliet and Jain (1)), is essential for the development, maintenance, progression, and metastasis of neoplastic tumors (2). Therefore, angiogenesis is considered to be the hallmark of cancerous tumors, and early detection of this process can facilitate the initiation of treatment and management of the disease (3). Although there are several known pro-angiogenic biomarkers, among these only endoglin (4), α_V_β_3_ integrin (5), and the vascular endothelial growth factor receptor 2 (VEGFR-2) (6) are well characterized and are overexpressed in many cancerous tumors, such as those of the breast, ovaries, and the pancreas (3). Endoglin (CD105) is a co-receptor of the transforming growth factor beta (TGF-β) and co-modulates the different activities, including angiogenesis, of the activated TGF-β receptor (7). The α_V_β_3_ integrin is a G-protein–coupled receptor that can bind several different ligands such as fibronectin, von Willebrand factor, fibrinogen, etc., and assists with the survival and migration of cancerous cells, which increases the invasive potential of cancerous cells, and promotes angiogenesis in tumors (8). The VEGFR-2 mediates its effects through a family of receptor tyrosine kinases that promote the mitogenesis, survival, differentiation, migration, and vascular permeability of endothelial cells (9).

Little information is available regarding the expression of the different angiogenic markers during the progression of a tumor from a small size to a larger size, and the noninvasive visualization of angiogenic markers that are overexpressed during initial stages of the neoplasia can facilitate early detection and treatment of the disease (3). For this, Deshpande et al. developed a series of microbubble (MB; perfluorocarbon gas enclosed within spherical lipid shells harboring streptavidin moieties to bind biotinylated monoclonal antibodies (mAb) directed toward specific targets)–based contrast agents that were coated with specific antibodies targeted to endoglin (MB_endoglin_), α_V_β_3_ integrin (MB_integrin_), and VEGFR 2 (MB_vegfr2_), respectively (3). The targeted MBs were then used with ultrasound imaging to determine the expression of the angiogenic antigens during the growth of human ovarian (SKOV3 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology)), human breast (MDA-MB-361 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-27&Template=cellBiology)), and human pancreatic (MiaPaCa2 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1420&Template=cellBiology)) cell line xenograft tumors in mice. This chapter describes the studies performed with MB_endoglin_. Studies performed with MB_integrin_ and MB_vegfr2_ are described in separate chapters of MICAD (www.micad.nih.gov) (10, 11).

### Related Resource Links

Microbubble related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Microbubbles+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books).

Homo sapiens endoglin transcript variant 1 protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001114753.1).

Endoglin in Online Mendelian Inheritance in Man (OMIM (http://omim.org/entry/131195)) Database.

Endoglin in Gene Expression Omnibus (GEO (http://www.ncbi.nlm.nih.gov/geo/info/profiles.html)) Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of MB_endoglin_ has been described in detail by Deshpande et al. (3). Briefly, the MBs were obtained as a freeze-dried preparation from a commercial source and reconstituted in 1 mL sterile 0.9% sodium chloride. Subsequently, 5 × 10^7^ of the reconstituted MBs were incubated with 5 μg biotinylated anti-mouse endoglin mAb for 10 min at room temperature to obtain MB_endoglin_. A similar procedure was used to obtain MB_integrin_ and MB_vegfr2_. For use as controls, another batch of MBs was linked to biotinylated rabbit immunoglobulin G antibodies (MB_control_). The procedure used to remove excess mAb, if any, from the final preparation was not reported. The average number of antibody molecules bound per square micrometer of the MBs was reported to be ~7,600 as determined with fluorescence-activated cell sorter analysis (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20in%20vitro%20studies&cmd=DetailsSearchhttp://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

A parallel plate flow chamber cell-binding assay with SVR cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2280&Template=cellBiology) (the high expression of endoglin and the other angiogenic biomarkers by these cells was confirmed with immunofluorescence staining) revealed that, compared to MB_control_, a significantly higher (P = 0.003) amount of MB_endoglin_ bound to these cells (3). Little or no binding of these MBs was observed with control cells (4T1 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology)) that did not express any of the angiogenic biomarkers. An overall significantly positive correlation (ρ = 0.83; P = 0.042) was observed between the number of MBs that attached to the SVR cells and the expression of endoglin by the cells. Pre-incubation of the SVR cells with the rabbit anti-mouse endoglin mAb was reported to block the binding of the MB_endoglin_.

An ex vivo immunofluorescence study of the tumor sections showed that endoglin in the cells was colocalized with CD31, a biomarker specific for endothelial cells (3). This indicated that the in vivo ultrasound signal obtained from the cancerous lesion was indeed generated by the MB_endoglin_ bound to the antigen expressed by the cells in the tumors. In addition, a good correlation (ρ = 0.88) was evident between the in vivo ultrasound imaging signal and the ex vivo expression level of endoglin in the tumors (P = 0.002) (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20rodentia&cmd=DetailsSearch)]

The expression of endoglin was investigated using MB_endoglin_ with ultrasound imaging during the different stages based on growth size (small, 50–150 mm^3^; medium, 150–250 mm^3^; large, >250 mm^3^) of subcutaneous breast, ovarian, and pancreatic cell line xenograft tumors in mice (n = 3 animals/tumor type) as described by Deshpande at al (3). In addition, the expression of endoglin was compared with that of α_V_β_3_ integrin and VEGFR-2 in these lesions.

The expression of endoglin was reported to be significantly higher (P ≤ 0.04) than that of α_V_β_3_ integrin and VEGFR-2 in the small and medium-sized breast cell line xenograft tumors in the mice (3). The expression levels of α_V_β_3_ integrin and VEGFR-2 in these lesions were approximately the same (P = 0.70), and the large tumors expressed similar levels of all the three antigens (P ≥ 0.08).

The expression level of endoglin in all sizes of the ovarian cell line xenograft tumors, as determined with ultrasound imaging using MB_endoglin_, was reported to be higher than that of either α_V_β_3_ integrin or VEGFR-2 (P ≤ 0.04) (3). No significant difference (P ≥ 0.40) was observed in the expression level of α_V_β_3_ integrin and VEGFR-2 in all sizes of the xenograft tumors.

In the pancreatic cell line xenograft tumors, the small lesions expressed higher levels of α_V_β_3_ integrin compared with either endoglin (P = 0.15) or VEGFR-2 (P = 0.07) (3). No significant difference in the expression level of the three antigens in the medium-sized tumors was observed. The large pancreatic lesions showed a significantly higher (P = 0.01) expression of endoglin compared with VEGFR2 but not α_V_β_3_ integrin (P = 0.22).

From these studies, the investigators concluded that the expression level of the different angiogenic markers varies with the growth stage of the tumor (3). They also concluded that targeted MB-based contrast agents can be used with ultrasound imaging to detect tumors in the early stages of growth in mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MB%20endoglin%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No Supplemental Information is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 De Bock K., Mazzone M., Carmeliet P. (2011). Antiangiogenic therapy, hypoxia, and metastasis: risky liaisons, or not?. Nat Rev Clin Oncol.
3 Deshpande N., Ren Y., Foygel K., Rosenberg J., Willmann J.K. (2011). Tumor angiogenic marker expression levels during tumor growth: longitudinal assessment with molecularly targeted microbubbles and US imaging. Radiology.
4 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
5 Cai W., Chen X. (2006). Anti-angiogenic cancer therapy based on integrin alphavbeta3 antagonism. Anticancer Agents Med Chem.
6 Shibuya M., Claesson-Welsh L. (2006). Signal transduction by VEGF receptors in regulation of angiogenesis and lymphangiogenesis. Exp Cell Res.
7 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
8 Wu G., Wang X., Deng G., Wu L., Ju S., Teng G., Yao Y., Liu N. (2011). Novel peptide targeting integrin alphavbeta3-rich tumor cells by magnetic resonance imaging. J Magn Reson Imaging.
9 Koch S., Tugues S., Li X., Gualandi L., Claesson-Welsh L. (2011). Signal transduction by vascular endothelial growth factor receptors. Biochem J.
10 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse alphaV beta3 integrin monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., Microbubbles coated with biotinylated rabbit anti-mouse vascular endothelial growth factor receptor 2 monoclonal antibody. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.